# ^99m^Tc-Labeled hydrazinonicotinamide-cysteine-annexin A5

Chemical name: | ^99m^Tc-Labeled hydrazinonicotinamide-cysteine-annexin A5
Abbreviated name: | ^99m^Tc-HYNIC-cys-Annexin A5
Synonym:
Agent Category: | Protein
Target: | Phosphatidylserine
Target Category: | Phospholipid
Method of detection: | Single photon emission computed tomography (SPECT); planar gamma imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals | Structural information is not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=annexin%20a5&cmd=DetailsSearch)]

The complex process of programmed cell death (apoptosis) has a very important function in the normal development and differentiation of tissues in animals (1). An increased rate of apoptosis can result in diseases of the cardiovascular (e.g., stroke, myocardial infarction, etc.), nervous (e.g., neurodegeneration), or immune (e.g., autoimmunity) systems, and the development of cancer is often attributed to a reduced rate of apoptosis (2, 3). A characteristic feature of apoptosis is the exposure of phosphatidylserine (PS), a negatively charged phospholipid that is usually present on the inner layer of the cell membrane, due to the process of membrane inversion observed during cell death (4). Also, annexin A5 (a 36-kD protein) is known to bind specifically to the exposed PS on apoptotic cell membranes (5) and it has been conjugated to a variety of nuclides or fluorescent dyes for the detection and visualization of apoptosis in tissues with different disease pathologies using scintigraphic and optical techniques (6).

^99m^Technetium-labeled hydrazinonicotinamide-annexin A5 (^99m^Tc-HYNIC-annexin A5) is a commonly used probe for the imaging of apoptotic tissue with single-photon emission computed tomography (SPECT) (3). To generate ^99m^Tc-HYNIC-annexin A5, the conjugation of HYNIC to annexin A5 is achieved by non-specifically directing HYNIC to an amino group on one of the 21 lysine residues in the protein structure, and any one of the lysine residues may bind the conjugating agent resulting in the formation of a molecule with an uncertain structure. In an effort to develop an annexin A5–based apoptosis imaging agent with a clear chemical structure, Fonge et al., using site-directed mutagenesis, incorporated a cysteine residue on the concave side of the protein to avoid altering the PS binding site on the convex side of the molecule (7) (for structural information of annexin, see van Genderen et al. (7)) and used the modified protein (cys-annexin A5) to generate HYNIC-cys-annexin A5 (3). HYNIC-cys-annexin A5 was subsequently labeled with ^99m^Tc (^99m^Tc-HYNIC-cys-annexin A5), and the biodistribution of this radiochemical was investigated in normal mice and compared to the biodistribution of ^99m^Tc-HYNIC-annexin A5 in another group of the same animals (3). ^99m^Tc-HYNIC-cys-annexin A5 uptake by the liver of mice treated with anti-Fas monoclonal antibody (anti-Fas mAb) was shown to detect the induced hepatic apoptosis in the animals. In another study, myocardial infarction in rabbits was visualized with ^99m^Tc-HYNIC-cys-annexin A5 using SPECT.

### Other sources of information regarding annexin V

Other chapters on annexin V in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=annexin+V+AND+micad%5Bbook%5D&doptcmdl=TOCView&log%24=booksrch&bname=micad).

Annexin V in OMIM (Online Mendelian Inheritance in Man) (http://www.ncbi.nlm.nih.gov/omim?term=annexin%20V).

Protein and nucleotide (mRNA) (http://www.ncbi.nlm.nih.gov/nuccore/NM_001154.3?ordinalpos=11&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) sequences of human annexin V.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-HYNIC-cys-annexin%20A5%20synthesis&cmd=DetailsSearch)]

The synthesis of ^99m^Tc-HYNIC-cys-annexin A5 was described by Fonge et al. (3). The labeling yield of this radiochemical was reported to be ≥90%. However, the purity, stability, and specific activity of the labeled protein were not reported. For comparative studies, ^99m^Tc-HYNIC-annexin A5 with a radiochemical yield of ≥90% was also synthesized by the investigators, but the purity, stability, and specific activity of this labeled compound was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-HYNIC-cys-annexin%20A5%20in%20vitro%20studies&cmd=DetailsSearch)]

No references are currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-HYNIC-cys-annexin%20A5%20rodentia&cmd=DetailsSearch)]

Fonge et al. compared the biodistribution of ^99m^Tc-HYNIC-cys-annexin A5 to that of ^99m^Tc-HYNIC-annexin A5 in normal mice (n = 4 animals/time point per labeled compound) (3). The animals (under anesthesia) were injected with the respective radiochemicals and euthanized at preset time points to determine the ex vivo biodistribution of radioactivity in the major organs. Although radioactivity from the two radiochemicals had a similar trend of biodistribution in the animals, some differences were apparent. At 10 min post-injection (p.i.), a significantly (P = 0.009) higher amount of radioactivity from ^99m^Tc-HYNIC-annexin A5 (56.9 ± 6.3% of injected dose/gram tissue (% ID/g)) was accumulated in the kidneys compared to that from ^99m^Tc-HYNIC-cys-annexin A5 (39.1 ± 6.9% ID/g), but at 60 min p.i., the amount of radioactivity accumulated in this organ from the two radiochemical was almost the same (P = 0.084). With ^99m^Tc-HYNIC-cys-annexin A5 (11.3 ± 0.5% ID/g at 10 min p.i. and 10.8 ± 1.0% ID/g at 60 min p.i.), a significantly (P = 0.0001) higher uptake of radioactivity by the liver was observed as compared to ^99m^Tc-HYNIC-annexin A5 (7.1 ± 0.5% ID/g at 10 min p.i. and 5.3 ± 0.7% ID/g at 60 min p.i.).

In another study to investigate the detection of apoptosis in the liver under in vivo conditions, mice with or without (controls) anti-Fas mAb treatment (to induce apoptosis in the liver) were injected with the respective tracers (n ≥ 3–4 mice/time point) 2 h after the mAb injection (3). At 1 h p.i., a significantly (P < 0.05) higher amount of radioactivity was observed in liver of the mAb-pretreated animals (43.1 ± 4.7% ID/g) with ^99m^Tc-HYNIC-cys-annexin A5 and ^99m^Tc-HYNIC-annexin A5 (35.0 ± 10.0% ID/g; these are only estimated values from Figure 3 of Fonge et al. (3)). In comparison, the control animals had an uptake of 19.0 ± 0.9% ID/g with ^99m^Tc-HYNIC-cys-annexin A5 and an estimated 9.0 ± 1.0% ID/g with ^99m^Tc-HYNIC-annexin A5 (from Figure 3 of Fonge et al. (3)). These observations were confirmed with ex vivo radioautography of livers obtained from the animals. Results obtained from this study indicated that, similar to ^99m^Tc-HYNIC-annexin A5, the uptake of ^99m^Tc-HYNIC-cys-annexin A5 was suitable for the detection of expression of PS in the mouse liver model.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-HYNIC-cys-annexin%20A5%20non%20primate%20mammals&cmd=DetailsSearch)]

Fonge et al. showed that microSPECT (μSPECT) imaging with ^99m^Tc-HYNIC-cys-annexinA5 could detect apoptosis at the site of induced myocardial infarction in rabbits (n = 3 animals) (3). The site of the infarct was confirmed using ^13^N-NH_3_ perfusion with micro positron emission tomography. From the μSPECT images it was reported that there was a 185 ± 57.6% increase in the uptake of ^99m^Tc-HYNIC-cys-annexin A5 at the affected area of the myocardium compared to the normal viable myocardium at 9 h p.i.

From these studies, the investigators concluded that introduction of a cysteine moiety into the concave side of the HYNIC-annexin A5 structure did not affect its ability to bind PS (3). In addition, ^99m^Tc- HYNIC-cys-annexin A5 could be used for the in vivo detection of apoptosis in two clinically relevant animal models.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-HYNIC-cys-annexin%20A5%20non%20human%20primates&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-HYNIC-cys-annexin%20A5%20human%20studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Zhao Y., Kuge Y., Zhao S., Strauss H.W., Blankenberg F.G., Tamaki N. (2008). Prolonged high-fat feeding enhances aortic 18F-FDG and 99mTc-annexin A5 uptake in apolipoprotein E-deficient and wild-type C57BL/6J mice. J Nucl Med.
2 Blankenberg F.G. (2008). In vivo detection of apoptosis. J Nucl Med.
3 Fonge H., de Saint Hubert M., Vunckx K., Rattat D., Nuyts J., Bormans G., Ni Y., Reutelingsperger C., Verbruggen A. (2008). Preliminary in vivo evaluation of a novel 99mTc-labeled HYNIC-cys-annexin A5 as an apoptosis imaging agent. Bioorg Med Chem Lett.
4 Blankenberg, F.G., Apoptosis Imaging: Anti-Cancer Agents in Medicinal Chemistry. Anticancer Agents Med Chem, 2009
5 Garnier B., Bouter A., Gounou C., Petry K.G., Brisson A.R. (2009). Annexin A5-functionalized liposomes for targeting phosphatidylserine-exposing membranes. Bioconjug Chem.
6 Faust, A., S. Hermann, S. Wagner, G. Haufe, O. Schober, M. Schafers, and K. Kopka, Molecular Imaging of Apoptosis In vivo with Scintigraphic and Optical Biomarkers - A Status Report. Anticancer Agents Med Chem, 2009
7 van Genderen H.O., Kenis H., Hofstra L., Narula J., Reutelingsperger C.P. (2008). Extracellular annexin A5: functions of phosphatidylserine-binding and two-dimensional crystallization. Biochim Biophys Acta.